# ^68^Ga-1,4,7-Triazacyclononane-1,4,7-triacetic acid-p-isothiocyanatobenzyl-vascular endothelial growth factor-121

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane-1,4,7-triacetic acid-p-isothiocyanatobenzyl- vascular endothelial growth factor-121
Abbreviated name: | ^68^Ga-NOTA-VEGF_121_, ^68^Ga-NOTA-p-Bn-SCN-VEGF_121_
Synonym:
Agent category: | Polypeptide
Target: | Vascular endothelial growth factor receptor (VEGFR)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF-A.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga-NOTA-VEGF)]

The vascular endothelial growth factor (VEGF) family is composed of five VEGF glycoproteins (VEGF-A, VEGF-B, VEGF-C, VEGF-D, and VEGF-E) and includes at least six isoforms of various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (1). VEGF-A is composed of VEGF_121_, VEGF_165_, and VEGF_189_ isoforms, which are secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin as other VEGF polypeptides do (2). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4) on endothelial cells. Several types of non-endothelial cells, such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells, also express VEGFRs (1).

VEGF is overexpressed in various tumor cells and tumor-associated endothelial cells (3). Among the isoforms of VEGF-A, VEGF_121_ is freely soluble while all VEGF_189_ is bound to the cell membrane or extracellular matrix (ECM). VEGF_165_ exhibits an intermediary behavior (i.e., partly diffusible and partly bound). Inhibition of VEGFR function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (4, 5). Radiolabeled VEGF has been developed as a single-photon emission computed tomography tracer for imaging solid tumors and angiogenesis in humans (6-8). VEGFR-2 has been shown to mediate most of the VEGF-A activation in tumor endothelial cells (9, 10). Kang et al. (11) prepared ^68^Ga-1,4,7-triazacyclononane-1,4,7-triacetic acid-p-isothiocyanatobenzyl-VEGF_121_ (^68^Ga-NOTA-VEGF_121_) for use with positron emission tomography (PET) imaging of VEGFR expression in nude mice bearing U87MG human glioblastoma xenografts.

### Related Resource Links:

- Chapters in MICAD (VEGFR (http://www.ncbi.nlm.nih.gov/books/?term=VEGFR+AND+micad%5Bbook%5D), VEGF (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=VEGF+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (VEGFR-1 (http://www.ncbi.nlm.nih.gov/gene/2321), VEGFR-2 (http://www.ncbi.nlm.nih.gov/gene/3791), VEGF (http://www.ncbi.nlm.nih.gov/gene/7422))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VEGFR-1 (http://www.ncbi.nlm.nih.gov/omim/165070), VEGFR-2 (http://www.ncbi.nlm.nih.gov/omim/191306), VEGF-A (http://www.ncbi.nlm.nih.gov/omim/192240))
- Clinical trials (VEGF (http://www.clinicaltrials.gov/ct2/results?term=VEGF))
- Drug information in FDA (VEGF (http://google2.fda.gov/search?q=VEGF%29+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga-NOTA-VEGF+synthesis)]

NOTA-VEGF_121_ was prepared by conjugation of p-SCN-Bn-NOTA to VEGF_121_ (4.9 nmol) in a 100:1 molar ratio at pH 9.5 for 18 h at room temperature (11). NOTA-VEGF_121_ was purified with column chromatography. There were 2.7 NOTA moieties per conjugate as determined with mass spectroscopy. NOTA-VEGF_121_ (0.35 nmol) was radiolabeled using ~185 MBq (5 mCi) ^68^GaCl_3_ in phosphate buffer (pH 6.0) for 30 min at room temperature. ^68^Ga-NOTA-VEGF_121_ was purified with a PD-10 column. Total preparation time of the tracer was ~60 min. The radiochemical yield was 40 ± 5%. The radiochemical purity was >98%. The specific activity of ^68^Ga-NOTA-VEGF_121_ was reported to be 243.1 ± 104.6 MBq/µmol (6.6 ± 2.8 mCi/µmol). ^68^Ga-NOTA-VEGF_121_ remained >95% intact in 50% bovine serum medium for 6 h at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga-NOTA-VEGF+in+vitro)]

Binding affinities of VEGF_121_ and NOTA-VEGF_121_ for mouse recombinant VEGFR-2 were determined with ^125^I-VEGF_121_ (11)_._ VEGF_121_ and NOTA-VEGF_121_ exhibited IC_50_ values of 1.40 ± 0.36 nM and 8.24 ± 3.35 nM, respectively. Cellular uptake of ^68^Ga-NOTA-VEGF_121_ (0.56 pM) was determined using human arterial endothelial cells (HAECs), with uptake values of 6.4% and 11.0% incubation dose at 1 h and 4 h after incubation at 37°C, respectively. Excess VEGF_121_ (100 nM) and anti-VEGFR-2 antibody (45.5 nM) inhibited the radioactivity in HAECs at 4 h by 32% and 49%, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga-NOTA-VEGF+rodentia)]

Kang et al. (11) studied the whole-body distribution of ^68^Ga-NOTA-VEGF_121_ in nude mice (n = 3) bearing human U87MG xenografts with the use of PET imaging at 1, 2, and 4 h after intravenous injection of 5.12 MBq (0.14 mCi) ^64^Cu-NOTA-VEGF_121_ (~25 pmol). The U87MG tumors were clearly visualized at 1–4 h after injection. The tumor accumulation of radioactivity levels were 2.43 ± 0.15% injected dose per gram (ID/g) at 1 h, 2.73 ± 0.32% ID/g at 2 h, and 2.97 ± 0.06% ID/g at 4 h. Tumor/muscle ratios were 2.58 and 2.95 at 1 h and 4 h, respectively. Co-injection with VEGF_121_ (3.5 nmol/mouse) inhibited accumulation of radioactivity in the U87MG tumors by 40% at 2 h (P < 0.01). The tumor/muscle ratios of the blocked mice were 1.78 and 1.95 at 1 h and 4 h, respectively.

Ex vivo biodistribution studies were performed in nude mice (n = 3/group) bearing human U87MG xenografts at 1, 2, and 4 h after injection of 4.8 MBq (0.13 mCi) ^68^Ga-NOTA-VEGF_121_ (~25 pmol) (11). The tumor accumulation of radioactivity levels were 1.46 ± 0.20% ID/g at 1 h, 1.84 ± 0.14% ID/g at 2 h, and 1.90 ± 0.02% ID/g at 4 h. Tumor/muscle ratios were 2.9, 3.2, and 3.1 at 1, 2, and 4 h, respectively. High radioactivity levels were observed in the liver (40.9% ID/g) and spleen (21.2% ID/g) at 2 h. The radioactivity levels in the blood (3.5% ID/g at 2 h) and kidney (3.2% ID/g at 2 h) were higher than that in the tumor but markedly lower than that in the liver and spleen. Co-injection with VEGF_121_ (3.5 nmol/mouse) inhibited accumulation of radioactivity in the U87MG tumors by 52% at 2 h (P < 0.01). The tumor/muscle ratio of the blocked mice was ~1 at 2 h. The ex vivo tumor biodistribution data are consistent with the in vivo PET tumor radioactivity levels. Immunohistostaining of tumor sections confirmed the co-localization of radioactivity to tumor endothelial cells expressing VEFGR-2 at 1–4 h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga-NOTA-VEGF+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga-NOTA-VEGF+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=68Ga-NOTA-VEGF+human)]

No publication is currently available.

## References

1 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
2 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
3 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
4 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
5 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
6 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
7 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
9 Folkman J. (2002). Role of angiogenesis in tumor growth and metastasis. Semin Oncol.
10 Ferrara N., Gerber H.P., LeCouter J. (2003). The biology of VEGF and its receptors. Nat Med.
11 Kang C.M., Kim S.M., Koo H.J., Yim M.S., Lee K.H., Ryu E.K., Choe Y.S. (2013). In vivo characterization of 68Ga-NOTA-VEGF121 for the imaging of VEGF receptor expression in U87MG tumor xenograft models. Eur J Nucl Med Mol Imaging.